# Poly(ethylene glycol)-b-poly(L-lysine)-gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid micelle

Chemical name: | Poly(ethylene glycol)-b-poly(L-lysine)-gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid micelle | [image]
Abbreviated name: | PEG-P(Lys-DOTA-Gd) | [image]
Synonym: | | [image]
Agent Category: | Nanoparticles | [image]
Target: | Non-targeted | [image]
Target Category: | Non-targeted | [image]
Method of detection: | Magnetic resonance imaging (MRI) | [image]
Source of signal / contrast: | Gd | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of PEG-P(Lys-DOTA-Gd) (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=polymeric%20micelle%20and%20MRI)]

Poly(ethylene glycol) (PEG)-b-poly(L-lysine) (P(Lys))-gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (Gd-DOTA) micelle, abbreviated as PEG-P(Lys-DOTA-Gd), is a Gd-based macromolecular contrast agent that has been developed by Shiraishi et al. for contrast-enhanced magnetic resonance imaging (MRI) (1).

Magnetization recovery in the longitudinal direction (T1) and magnetization decay in the transverse plane (T2, T2*) form the basis of soft-tissue contrast in MRI (2). Use of Gd-based contrast agents results in a decrease of T1 and thus leads to positive contrast enhancement in MR images. However, to date, the US Food and Drug Administration-approved Gd-based agents such as Gd-diethylenetriamine pentaacetic acid (Gd-DTPA) are low-molecular-weight Gd-chelates that induce a relatively low T1 relaxivity (r_1_) because of their fast rotation. Their typical r_1_ values are in the range of 3–5 (mM·s)^-1^ (2). Macromolecular Gd-chelates have been developed to improve the r_1,_ and are often synthesized with PEG, P(Lys), poly(glutamic acid), dendrimers, liposomes, or dextrans (3-5). The large size of these macromolecular systems results in a higher r_1_ value because of the slow tumbling of macromolecules. In animals, these macromolecular agents exhibit a long circulation time in the bloodstream and accumulate preferentially within tumors (6). However, agents with high molecular weights may fail to be excreted from the body, and a high blood concentration could result in undesirably high background (5).

Shiraishi et al. synthesized two types of polymeric micelle–based MRI contrast agents through conjugation of a PEG-P(Lys) block copolymer and a Gd-DOTA chelate (1, 5). One type possesses only DOTA-substituted lysine residues, and the other possesses both DOTA-substituted and unmodified lysine residues. These agents have been designed on the basis of the concept that stable Gd-chelated block copolymers produce a high r_1_, whereas formation of complex micelles lowers the r_1_ (1, 5, 7, 8). In blood circulation, the agent presents as polymeric micelles, and the r_1_ is suppressed to a low level. The micelle structure inhibits access of water molecules to Gd ions in the inner core of polymeric micelles. In contrast, the polymeric micelles are gradually dissociated into single-polymer chains at the tumor sites. Because water molecules can easily access the Gd ions, the accumulated single-polymer chains generate a higher r_1_. Thus the micelle agent exhibits changeable r_1_via the formation and dissociation of micelle structure. In addition, a single block copolymer with a molecular weight of <30,000 can be excreted via the kidneys, thus minimizing the potential toxicity of the agents.

The PEG-P(Lys-DOTA) system developed by Shiraishi et al. has multiple units of DOTA-bound lysine moiety (1, 5). A fully DOTA-substituted block copolymer forms polymeric micelles, whereas insufficient DOTA conjugation to lysine residues prevents the formation of a polymeric micelle. In other words, the micelle structures do not form in the presence of a small amount of unmodified lysine residue. The Gd ion is only partially chelated to DOTA (20% of vacant DOTA) in the block copolymer even excess amount of Gd ions was added to the block copolymer because DOTA–DOTA interactions prevent the Gd ion from freely chelating into a DOTA moiety. Gd-Chelated PEG-P(Lys-DOTA-Gd) could maintain the polymeric micelle structure. Therefore, the formation of the polymeric micelle appears to depend on interactions among vacant DOTAs. In addition, DOTA has been selected instead of DTPA because DOTA forms a more thermodynamically stable and kinetically inert complex than DTPA. The combination of PEG-P(Lys) copolymers and DOTA gives a more facile synthesis and a more stable metal chelation. Shiraishi et al. tested two micelle-based agents: PEG-P(Lys-DOTA-Gd) and PEG-P(Lys-DOTA-Gd)-dextran sulfate (PIC) micelles (1, 5). This chapter summarizes the data obtained with PEG-P(Lys-DOTA-Gd) micelles. Another chapter summarizes the data obtained with PIC micelles (http://www.ncbi.nlm.nih.gov/books/NBK5330/).

### Related Resource Links:

- Agents synthesized with polymeric materials in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=polymer+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Nanoparticle agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=nanoparticles+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19331861)]

Shiraishi et al. described the synthesis of PEG-P(Lys-DOTA-Gd) in detail (1). PEG-P(Lys-DOTA) was synthesized by means of polymerization of ε-(benzyloxycarbonyl)-L-lysine N-carboxyanhydride from PEG-NH_2_. The desired DOTA moiety numbers in PEG-P(Lys-DOTA) were controlled via adjustment of the DOTA-OSu/polymer ratio. Gd-Chelation was induced by mixing GdCl_3_·6H_2_O and PEG-P(Lys-DOTA) to produce PEG-P(Lys-DOTA-Gd).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19331861)]

In vitro characterization showed that the obtained PEG-P(Lys-DOTA-Gd) micelles had 118 ethylene glycol units, 17 lysine units, 17 DOTA conjugated to lysine residues, and 7 Gd ions, which was coded as 118-17-17-7 (1). This micelle had a weight average of 42.9 ± 7.6 nm, accompanied by a secondary aggregation of a weight average of 225.5 ± 53.0 nm. The size of the micelles was 50–250 nm in diameter. The zeta-potential was −9.55 mV in 150 mM NaCl solution, indicating that the polymeric micelle was negatively charged.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19331861)]

Pharmacokinetic studies (n = 1 mouse) showed that accumulation of the PEG-P(Lys-DOTA-Gd) micelle remained at 22.5 ± 2.9% injected dose (ID) and 10.2 ± 1.4% ID (n = 3 blood samples) in blood at 24 h and 48 h after tail vein injection, respectively, indicating that the micelle was highly stable in blood (1). In contrast, the low-molecular-weight Gd-DTPA was immediately excreted 1 h after injection (only 1.4 ± 0.8% ID was found in blood).

Biodistribution of the PEG-P(Lys-DOTA-Gd) micelle was evaluated in CDF1 female mice bearing colon 26 tumors (1). Accumulation of the micelle in tumor tissues reached 6.1 ± 0.3% ID/g tissue at 24 h after injection. Low accumulation was also observed in heart, kidneys, and muscle tissue at the same time point. High accumulation was found in liver (10.8 ± 0.9% ID/g) and spleen (7.2 ± 0.7% ID/g) at 24 h after injection. In urine, 20.8 ± 7.6% ID of the polymeric micelle was found at 48 h after injection. The polymeric micelle was excreted through the kidney filtration in a dissociated polymer form.

T1-Weighted MR images before injection and 24 h after injection showed a clear signal enhancement (a two-fold increase) in the tumor compared with the signal before injection (1). The signal intensity in the tumor increased gradually by 24 h and then decreased slightly by 48 h. However, even at 24 h after the injection, an intense signal was observed in the heart and aorta areas. This suggests that a considerable amount of the contrast agent was circulating in the bloodstream. Apparent signal enhancement was also observed in the kidneys, indicating that the kidneys excreted the contrast agent. To estimate possible acute toxicity, a dose four times that of the original agent volume was injected into the mouse tail vein, and there was no significant difference for the body weight over 16 days in comparison to the control (less than ± 10%) (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Shiraishi K., et al. (2009). Preparation and in vivo imaging of PEG-poly(L-lysine)-based polymeric micelle MRI contrast agents. J Control Release.
2 Makowski M.R., et al. (2009). Molecular imaging with targeted contrast agents. Top Magn Reson Imaging.
3 Torchilin V.P. (2000). Polymeric contrast agents for medical imaging. Curr Pharm Biotechnol.
4 Torchilin V.P. (2002). PEG-based micelles as carriers of contrast agents for different imaging modalities. Adv Drug Deliv Rev.
5 Shiraishi K., et al. (2010). Polyion complex micelle MRI contrast agents from poly(ethylene glycol)-b-poly(l-lysine) block copolymers having Gd-DOTA; preparations and their control of T(1)-relaxivities and blood circulation characteristics. J Control Release.
6 Ma H., et al. (2010). Accelerated blood clearance was not induced for a gadolinium-containing PEG-poly(L-lysine)-based polymeric micelle in mice. Pharm Res.
7 Nakamura E., et al. (2006). A polymeric micelle MRI contrast agent with changeable relaxivity. J Control Release.
8 Bae Y., Kataoka K. (2009). Intelligent polymeric micelles from functional poly(ethylene glycol)-poly(amino acid) block copolymers. Adv Drug Deliv Rev.